# ^68^Ga-Labeled 2-{3-[5-(7-{1-benzyloxycarbonyl-5-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]pentylcarbamoyl}-heptanoylamino)-1-carboxypentyl]ureido}pentanedioic acid

Chemical name: | ^68^Ga-Labeled 2-{3-[5-(7-{1-benzyloxycarbonyl-5-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]pentylcarbamoyl}-heptanoylamino)-1-carboxypentyl]ureido}pentanedioic acid
Abbreviated name: | [^68^Ga]3
Synonym:
Agent Category: | Compound
Target: | Prostate-specific membrane antigen (PSMA)
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information on [^68^Ga]3 in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=psma%20and%20prostate%20cancer&cmd=DetailsSearch)]

The prostate-specific membrane antigen (PSMA) is a type II membrane glycoprotein that is present primarily in the prostate and is overexpressed during all stages of the androgen-insensitive or the metastatic cancer of this organ (1). In addition, PSMA is expressed at lower levels (compared to the prostate) in the neovasculature of some solid tumors (for details, see Elsasser-Beile et al. (1)). Because of its high expression during the development and progression of a malignancy, PSMA is considered to be a good target for the imaging and treatment of prostate cancer (2). Several investigators have reported the use of radio-halogenated (e.g., ^18^F, ^125^I, etc.) and ^99m^Tc-labeled small molecule inhibitors for the imaging of PSMA (3). Among these radionuclides, ^18^F is the most frequently used to label diverse positron emission tomography (PET) agents for diagnostic imaging because its addition to a molecule (usually by the replacement of a hydrogen atom) does not alter its chemical properties; however, due to its short half-life (~110 min), an on-site cyclotron is needed to produce this radio-halogen (4). Recently ^68^Ga (half-life, ~68 min) has been suggested to be a suitable alternative to the use of ^18^F for the production of PET imaging probes because ^68^Ga is easy to produce with a ^68^Ge/^68^Ga generator system that does not have to be on-site. However, it is necessary to mention that currently no ^68^Ge/^68^Ga generator system has been approved by the United States Food and Drug Administration (Eckelman: personal communication). In addition, ^68^Ga has been successfully used by some investigators to study cancer and tumor biology (4, 5). On the basis of these observations, and as an extension of their earlier work (for references, see Banerjee et al. (3)), Banerjee et al. developed two ^68^Ga-labeled, urea-based inhibitors of PSMA ([^68^Ga]-labeled 2-{3-[5-(7-{1-benzyloxycarbonyl-5-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]pentylcarbamoyl}-heptanoylamino)-1-carboxypentyl]ureido}pentanedioic acid ([^68^Ga]3) and [^68^Ga]-labeled 2-[3-(1-carboxy-5-{7-[5-carboxy-5-(3-phenyl-2-{3-phenyl-2-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]propionylamino}propionylamino)pentylcarbamoyl]heptanoylamino}pentyl)

ureido]pentanedioic acid ([^68^Ga]6)) and evaluated them for biodistribution and the imaging of PSMA-expressing tumors in nude mice (3). This chapter details the results obtained with [^68^Ga]3. Results obtained with [^68^Ga]6 are presented in a separate chapter of MICAD (www.micad.nih.gov) (6).

### Other Sources of Information

PSMA-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=PSMA+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad).

Alternate names and other information regarding PSMA in the Human Protein Reference Database (http://www.hprd.org/alternate?hprd_id=02961&isoform_id=02961_1&isoform_name=Isoform_1).

Clinical trials (http://clinicaltrials.gov/ct2/results?term=PSMA) involving PSMA and PSMA inhibitors.

Gene information (Gene ID: 2346) for human PSMA in Entrez Gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=2346).

PSMA1 variant 3 Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_001193471.1).

Information on PSMA in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/omim/600934).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B68Ga%5D3%20synthesis&cmd=DetailsSearch)]

The synthesis of [^68^Ga]3 has been described in detail by Banerjee et al. (3). The radiochemical yield and purity of the labeled compound were reported to be 76.2% and >99.0%, respectively. The retention time of [^68^Ga]3 on analytical high-performance liquid chromatography (HPLC) was 25.0 min compared with a retention time of 22.5 min for [^68^Ga]6. The specific activity of [^68^Ga]3 was reported to be between 3.0 and 6.0 MBq/nmol (81 and 162 μCi/nmol). After purification, the radiochemical was dried under vacuum and diluted in 0.9% saline to the desired tracer concentration before use in biodistribution and imaging studies. The stability of [^68^Ga]3 under in vitro or in vivo conditions was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga-3%20in%20vitro&cmd=DetailsSearch)]

Using unlabeled 3 and [^68^Ga]3 in a fluorescence-based PSMA inhibition assay, the inhibitory concentrations of these compounds were reported to be 2.9 and 29.0 nM, respectively (3). In comparison, the PSMA inhibitory concentrations for unlabeled 6 and [^68^Ga]6 were 1.23 and 0.44 nM, respectively.

Using a 1-octanol/water system, the partition coefficient of [^68^Ga]3 was determined to be −3.9, which was similar to that of [^68^Ga]6 (3). This indicated that both radiolabeled compounds were lipophilic (3). On the basis of the HPLC analysis reported above, [^68^Ga]6 appeared to have a slightly higher lipophilicity than [^68^Ga]3.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

The biodistribution of [^68^Ga]3 was studied in severe-combined immunodeficient mice bearing PC-3 (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1435&Template=cellBiology)-PIP (transfected with the PSMA gene and expressing high levels of the antigen) and PC-3-FLU (does not express PSMA) cell xenograft tumors (3). The mice were injected with the tracer through the tail vein and euthanized 30, 60, 120, and 180 min after the injection (n = 4 mice/time point) to determine the amount of radioactivity accumulated in the tumors and major organs. Results obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). At 30 min post-injection (p.i.), the PC-3-PIP tumors had an uptake of 3.78 ± 0.09% ID/g that reduced gradually to 1.10 ± 0.19% ID/g by 3 h p.i.; uptake in the PC-3-FLU tumors was 0.82 ± 0.20% ID/g at 30 min p.i. and 0.39 ± 0.02% ID/g at 3 h p.i. During the same period, the label cleared rapidly from the kidneys, with an uptake of 97.19 ± 16.07% ID/g at 30 min p.i. that decreased to 2.13 ± 0.11% ID/g at 3 h p.i. Except for the bladder, all other organs had <1.0% ID/g incorporation of radioactivity by 3 h p.i. The accumulation of radioactivity in the bladder was 8.96 ± 5.30% ID/g at 30 min p.i., and this increased to 25.29 ± 8.63% ID/g at 60 min p.i. and decreased to 5.39 ± 2.98 at 3 h p.i. This indicated that the tracer was excreted mainly through the urinary route. The PC-3-PIP tumor/muscle uptake ratio (T/M) increased from 8.30 at 30 min p.i. to 20.37 at 3 h p.i. In comparison, the T/M for the PC-3-FLU tumors was 1.80 at 30 min p.i. and increased to 7.34 at 3 h p.i. In mice injected with [^68^Ga]6 PC-3-PIP, the T/M ratio was 4.17 at 30 min p.i. and increased to 436.29 at 3 h p.i.; during the same time, the PC-3-FLU T/M ratio increased from 1.67 at 30 min p.i. to 28.70 at 3 h p.i. in these animals (for other details on [^68^Ga]6, see the related chapter in MICAD (6)).

For the PET imaging study, a single animal bearing LNCaP (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1740&Template=cellBiology) cell (expressing PSMA) tumors was injected intravenously with either [^68^Ga]3 or [^68^Ga]6 as described by Banerjee et al. (3). From the PET images it was clear that both tracers accumulated primarily in the PSMA-positive tumors and the kidneys (the kidneys are known to express PSMA in the proximal renal tubules), similar to observations made during the biodistribution study. In a blocking study, the tumor-bearing mice (number of mice used per time point was not reported) were injected with 2-(phosphonomethyl)pentanedioic acid (2-PMPA) (50 mg/kg body weight), a known selective ligand of PSMA, and later the animals were injected with the respective tracers (time elapsed between the pretreatment with 2-PMPA and injection of the tracer was not reported). PET images of the animals were acquired at 30 and 60 min p.i., and it was observed that the PSMA-expressing tumors and the kidneys did not accumulate either tracer, suggesting that both radiochemicals bound specifically to the membrane antigen.

From these studies, the investigators concluded that both [^68^Ga]3 and [^68^Ga]6 bind specifically to PSMA and could be used for the imaging of PSMA-positive tumors in rodents (3). They also mentioned that more animal studies are necessary before these radiochemicals can be evaluated in the clinic.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga-3%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga-3%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=68Ga-3%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were funded by National Institutes of Health grants R01CA134675 and U24 CA92871.

## References

1 Elsasser-Beile U., Buhler P., Wolf P. (2009). Targeted therapies for prostate cancer against the prostate specific membrane antigen. Curr Drug Targets.
2 Dijkgraaf I., Boerman O.C. (2009). Radionuclide imaging of tumor angiogenesis. Cancer Biother Radiopharm.
3 Banerjee S.R., Pullambhatla M., Byun Y., Nimmagadda S., Green G., Fox J.J., Horti A., Mease R.C., Pomper M.G. (2010). 68Ga-labeled inhibitors of prostate-specific membrane antigen (PSMA) for imaging prostate cancer. J Med Chem.
4 Fani M., Andre J.P., Maecke H.R. (2008). 68Ga-PET: a powerful generator-based alternative to cyclotron-based PET radiopharmaceuticals. Contrast Media Mol Imaging.
5 Holland J.P., Williamson M.J., Lewis J.S. (2010). Unconventional nuclides for radiopharmaceuticals. Mol Imaging.
6 Chopra, A., [68Ga]-Labeled 2-[3-(1-Carboxy-5-{7-[5-carboxy-5-(3-phenyl-2-{3-phenyl-2-[2-(4,7,10-tris-carboxymethyl-1,4,7,10-tetraazacyclododec-1-l)acetylamino]propionylamino}propionylamino)pentylcarbamoyl]heptanoylamino}pentyl)ureido]pentanedioic Acid. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.